# Perfluoropolyethylene glycol–labeled BDC2.5 T cells

Chemical name: | Perfluoropolyethylene glycol–labeled BDC2.5 T cells
Abbreviated name: | PFPE-BTCs
Synonym:
Agent category: | Labeled cell
Target: | Other
Target Category: | Other –inflamed tissue
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal/contrast: | ^19^F
Activation: | No
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=PFPE + T cells)]

T cells (TCs) are responsible for regulating immune responses and maintaining immune tolerance via recognition of peptide antigens that are bound to human leukocytes (1). Some TCs possess autoimmunity or self-tolerance through recognition of self-antigens. Loss of this required self-tolerance can result in an autoimmune disorder. For example, type 1 diabetes (T1D) is characterized by a spontaneous loss of immunological tolerance of pancreatic β-cells, which leads TCs to attack insulin-producing β-cells in the islets of Langerhans in the pancreas (2). The development of T1D has two stages: the insulitis phase when mixed leukocytes invade the islets and destroy β-cells, and the diabetes phase when the bulk of β-cells (up to 90%) have been destroyed and no longer produce sufficient insulin to control blood glucose levels (2). These stages can be reproduced easily in the non-obese diabetic (NOD) mouse model for human T1D (3), a spontaneous murine model in which insulitis and diabetes appear mainly in females in ~5 and ~13 weeks, respectively (4). Studies in NOD mice demonstrate that the islets in the pancreas are infiltrated with autoreactive CD4^+^ TCs as majority cells, as well as other cells such as CD8^+^ TCs, dendritic cells, B cells, and macrophages, in the insulitis phase (3). From the spleen and lymph nodes of female NOD mice, islet antigen-specific TCs, known as BDC2.5 TCs (BTCs), are derived and identified to be diabetogenic CD4^+^ TCs (5). Adoptive transfer of BTCs to NOD severe combined immunodeficiency (SCID) mice can accelerate diabetes (6). Expressing TC receptor genes (TCR) of BTCs in transgenic (Tg) mice produce a murine model (BDC2.5 TCR Tg/NOD SCID mice) with monoclonal TC repertoire in which all of the TCs are CD4^+^ type (5). Imaging these TCs in the progression of T1D is important to the understanding of the pathogenesis of autoimmunity and to the design of immunotherapeutic interventions (6).

Being the only stable isotope of fluorine with a natural abundance of ~100%, ^19^F has a nuclear spin 1/2 with a large gyromagnetic ratio (γ ~40.05 MHz/T) (7). The small γ difference between the ^19^F and ^1^H (~6%) allows the use of existing proton nuclear magnetic resonance (NMR) instrumentation with minor adjustments to detect fluorinated species at high sensitivity (~83% relative to ^1^H). Endogenous fluorine in vivo is found primarily in bones and teeth as solid fluorides, which have very short T_2_ relaxation times and result in an undetectable signal with magnetic resonance imaging (MRI). Therefore, exogenously administered fluorinated tracers can be used to track various biological processes in vivo. For example, perfluorocarbons (PFC) such as perfluoro-15-crown-5 (15C5) have been used to measure oxygen tensions in tissues and tumors (8) and to label dendritic cells (9). The lack of background ^19^F signal is advantageous in in vivo applications, but additional ^1^H images are required to provide anatomic interpretations. PFCs are extremely hydrophobic and do not dissolve in blood directly; they normally are formulated as biocompatible emulsions for intravenous administration (7). Inside the body, the PFC particles are cleared from circulation by phagocytes/macrophages and/or by respiration within several hours or days, depending on the administered dose, particle size, and PFC (10). Many commercial PFC emulsions have been found to be nontoxic or do not cause any health problems other than tissue swelling (7). Perfluoropolyethylene glycol (PFPE, Mw 1750) is a linear PFC that contains a large number of ^19^F atoms per molecule for enhancing sensitivity (6). The center CF_2_ groups can generate a strong peak (>0.9 at -92 ppm) that dominates 90% of its ^19^F signal, whereas the end CF_2_ groups yield a weak signal (<0.1 at -79 ppm) that is below the in vivo MRI detection limit. The spin relaxation time (T_1_) is 2.2 times shorter than that of 15C5 at 11.7 T, which allows a shorter imaging acquisition time. PFPE can be emulsified to form particles ~100–200 nm in diameter, allowing for cellular uptake via endocytosis (9). BTCs are labeled with PFPE (PFPE-BTCs) for ^19^F MRI.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( PFPE + T cells)+AND+synthesis%0D%0A)]

Srinivas et al. briefly described the detailed preparation of PFPE-BTCs (6). First, commercially available PFPE was emulsified with commercially available surfactant poloxamers at a molar ratio of 1:1 to produce PFPE nanoparticles 103 ± 4 nm in diameter. Poloxamers are nonionic triblock copolymers composed of a central hydrophobic chain of polyoxypropylene flanked by hydrophilic chains of polyoxyethylene. TCs derived from the BDC2.5 TCR Tg mouse were activated in vitro in the presence of 1 μg/mL anti-CD28 and 10 U/mL IL-2, followed by incubation with PFPE emulsion and the commercial transfection agent FuGEN 6 for 3.5 h at 37°C to yield PFPE-BTCs. PFPE was found to exhibit 2.2 × 10^13^ fluorine spins per TC as determined by ^19^F NMR. The chemical shifts were found to be -92 ppm for the major peak (central CF_2_ groups) and -79 ppm for the minor peak (end CF_2_ group).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( PFPE + T cells)+AND+%22in+vitro%22)]

The effects of PFPE on cytotoxicity, cellular viability, and phenotype of labeled BTCs were examined in vitro (6). A Trypan blue exclusion assay was used to evaluate the cytotoxicity of PFPE. No apparent cytotoxicity was found for all conditions studied. A methyl thiazole tetrazolium assay was used to determine the cellular viability, which was ~95% 2–48 h after labeling. Flow cytometry was used to assess several cellular surface markers in the BTCs, including CD62L (a lectin-binding protein) and CD4 (a major histocompatibility complex (MHC) II-interacting co-receptor). No apparent downregulation was found in the expression of CD62L in the labeled cells compared with that in the unlabeled cells, which suggests that the labeling with PFPE emulsions did not appear to activate naïve TCs. A transient reduction of CD4 expression was observed in the presence of transfections agents, which was related to the receptor-mediated endocytosis of PFPE nanoparticles. The cellular internalization was examined with PFPE emulsions labeled with the fluorescent probe dialkylcarbocyanine dye (DiI) via fluorescence microscopy. The fluorescence-labeled PFPE appeared to bind to the cell membrane or to be localized within the cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( PFPE + T cells) +AND++rodentia)]

Srinivas et al. examined the migration of PFPE-BTCs in mice with in vivo ^19^F MRI/^1^H MRI (6). NOD SCID mice (8–10 weeks old, n = 4) received intraperitoneal injections of 4 × 10^6^ PFPE-BTCs and imaged 48 h later with an 11.7-T (^19^F resonant frequency 470 MHz) NMR spectrometer. The ^19^F images demonstrated a localized signal in the region of the pancreas but not in the liver or spleen. This result was further confirmed with histological analysis of pancreas. TCs were found around the islet in the pancreas 24 h after adoptive transfer of PFPE-BTCs, suggesting that the labeled TCs were capable of homing to the pancreas in vivo. From the in vivo ^19^F images, the number of detected TCs in the pancreas was quantified as 1.5% to 3.4% of the total transferred cells with the average cell density of ~28,000 cells per voxel, which was verified to be 2.9 ± 0.3% with ex vivo ^19^F NMR. The majority of transferred cells remained at the injection site or circulating in the body, and their concentrations were too low to be detected with in vivo ^19^F MRI. As controls, PFPE emulsions or labeled non-specific TCs (MHC-mismatch non-specific TCs derived from MHC-mismatched BLAB/c mice) were intraperitoneally injected into NOD SCID mice, and the ^19^F images were collected 48 h later. For PFPE emulsions, some ^19^F signal was found in the abdominal cavity near the bladder but not in pancreas. For the non-specific TCs, no ^19^F signal was found in or around the pancreas.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( PFPE + T cells) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( PFPE + T cells) +AND+human)]

No publication is currently available.

### NIH Support

EB004155, HD047675, ES012359, EB001977

## References

1 Hohlfeld R. Meinl E. Weber F. Zipp F. Schmidt S. Sotgiu S. Goebels N. Voltz R. Spuler S. Iglesias A. The role of autoimmune T lymphocytes in the pathogenesis of multiple sclerosis Neurology 1995 45Suppl 66 S33 8 7783909
2 Denis M.C., Mahmood U., Benoist C., Mathis D., Weissleder R. (2004). Imaging inflammation of the pancreatic islets in type 1 diabetes. Proc Natl Acad Sci U S A.
3 Brodie G.M., Wallberg M., Santamaria P., Wong F.S., Green E.A. (2008). B-cells promote intra-islet CD8+ cytotoxic T-cell survival to enhance type 1 diabetes. Diabetes.
4 Miyazaki A., Hanafusa T., Yamada K., Miyagawa J., Fujino-Kurihara H., Nakajima H., Nonaka K., Tarui S. (1985). Predominance of T lymphocytes in pancreatic islets and spleen of pre-diabetic non-obese diabetic (NOD) mice: a longitudinal study. Clin Exp Immunol.
5 Dobbs C., Haskins K. (2001). Comparison of a T cell clone and of T cells from a TCR transgenic mouse: TCR transgenic T cells specific for self-antigen are atypical. J Immunol.
6 Srinivas M., Morel P.A., Ernst L.A., Laidlaw D.H., Ahrens E.T. (2007). Fluorine-19 MRI for visualization and quantification of cell migration in a diabetes model. Magn Reson Med.
7 Yu J.X., Kodibagkar V.D., Cui W., Mason R.P. (2005). 19F: a versatile reporter for non-invasive physiology and pharmacology using magnetic resonance. Curr Med Chem.
8 Zhang W., Ito Y., Berlin E., Roberts R., Berkowitz B.A. (2003). Role of hypoxia during normal retinal vessel development and in experimental retinopathy of prematurity. Invest Ophthalmol Vis Sci.
9 Ahrens E.T., Flores R., Xu H., Morel P.A. (2005). In vivo imaging platform for tracking immunotherapeutic cells. Nat Biotechnol.
10 Noth U., Morrissey S.P., Deichmann R., Jung S., Adolf H., Haase A., Lutz J. (1997). Perfluoro-15-crown-5-ether labelled macrophages in adoptive transfer experimental allergic encephalomyelitis. Artif Cells Blood Substit Immobil Biotechnol.